# ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-conjugated dimeric [Tyr^3^]octreotide

Chemical name: | ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-conjugated dimeric [Tyr^3^]octreotide
Abbreviated name: | ^111^In-Dimeric [Tyr^3^]octreotide
Synonym:
Agent Category: | Peptides
Target: | Somatostatin receptors (SSTRs)
Target Category: | Receptors
Method of detection: | Single-photon emission computed tomography (SPECT) and planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | For structures of octreotide analogues, click on PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance?term=octreotide).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=somatostatin+receptor+and+targeted)]

The ^111^In-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-conjugated dimeric [Tyr^3^]octreotide, abbreviated as ^111^In-dimeric [Tyr^3^]octreotide, is an octreotide-based agent developed by Yim et al. for somatostatin receptor (SSTR)–targeted imaging and radionuclide therapy (1).

The human SSTR family is a group of G-protein–coupled receptors with five members (SSTR1–SSTR5). All receptor members have seven α-helical transmembrane domains and possess a highly conserved sequence motif (YANSCANPI/VLY) in the seventh topology, which serves as a signature sequence for this family (2-4). Overall, there is 39%–57% sequence identity among the members, with the highest homology between SSTR1 and SSTR4, and among SSTR2, SSTR3, and SSTR5, respectively. The two groups of receptors also differ in their interactions with somatostatin (SST) and its analogs. SSTR2, SSTR3, and SSTR5 have a high affinity for octreotide and seglitide, whereas SSTR1 and SSTR4 exhibit a very low affinity for them (1-3). With the exception of SSTR2, the precise contributions of other members remain to be elucidated. This is largely due to the lack of highly selective ligands and the co-expression of different subtypes in single cells. SSTRs are distributed widely in cells both in the nervous system and periphery, and they have been shown to be overexpressed in a large number of malignancies, with particularly high density in neuroendocrine tumors (5-7).

As the targets of SST radiopharmaceuticals, SSTRs are of considerable clinical relevance for tumor imaging and radionuclide therapy (4, 6, 8, 9). Because the native SST has a very short biological half-life (<2 min), various analogs have been synthesized, including octreotide, lanreotide, vapreotide, and their derivatives (6, 8, 10). In general, these analogs have a high affinity to SSTR2, somewhat lower affinity to SSTR3 and SSTR5, and almost no affinity to SSTR1 and SSTR4. Treatment with the radiolabeled analogs results in reduced hormonal overproduction and symptomatic relief in most patients with neuroendocrine tumors; however, it is much less successful in tumor size reduction (11, 12). Imaging with ^111^In-, ^90^Y-, or ^177^Lu-labeled [DOTA^0^,Tyr^3^]octreotide analogs has proven the usefulness of octreotide conjugates in the diagnosis and staging of neuroendocrine tumors (8, 9, 13).

There is growing interest in the development of polyvalent ligands for dual imaging and therapeutic purposes, considering that polyvalent ligands may have a higher binding affinity than monovalent analogs. Yim et al., synthesized mono-, di-, and tetrameric [Tyr^3^]octreotide conjugates with a two-stage metal-free ligation procedure (1). The investigators characterized these conjugates and compared them with ^111^In-labeled [DOTA^0^,Tyr^3^]octreotide ([^111^In-DOTA^0^,Tyr^3^]octreotide), a chemically engineered and long-acting analog. [^111^In-DOTA^0^,Tyr^3^]octreotide has been applied for imaging and treatment in patients with neuroendocrine tumors (6, 11, 12). Yim et al. have shown that the ^111^In-labeled monomeric and dimeric [Tyr^3^]octreotides, but not the tetrameric [Tyr^3^]octreotide, have a similar binding affinity for SSTRs and a longer tumor retention time when compared with [^111^In-DOTA^0^,Tyr^3^]octreotide (1). This chapter describes the results obtained with ^111^In-dimeric [Tyr^3^]octreotide.

### Related Resource Links:

- MICAD chapters on SSTR imaging (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=somatostatin+receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information on SSTRs (http://www.ncbi.nlm.nih.gov/gene/?term=somatostatin+receptors)
- Articles on SSTRs in Online Mendelian Inheritance in Man (OMIM (http://www.ncbi.nlm.nih.gov/omim?term=somatostatin%20receptors))
- Somatostatin analogues in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pccompound&term=somatostatin)
- Bioassays of SSTRs in PubChem (http://www.ncbi.nlm.nih.gov/pcassay?term=somatostatin%20receptors)
- SSTR-related clinical trials in ClinicalTrial.gov (http://clinicaltrials.gov/ct2/results?term=somatostatin+receptors)
- FDA-approved octreotide agents: Octreotide acetate (http://www.accessdata.fda.gov/scripts/cder/drugsatfda/index.cfm) and Octreoscan (http://www.accessdata.fda.gov/scripts/cder/drugsatfda/index.cfm?fuseaction=Search.DrugDetails)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20411957)]

DOTA-conjugated dimeric [Tyr^3^]octreotide was synthesized with a two-stage ligation procedure that combined the Cu(I)-catalyzed “click” reaction between dendrimeric alkynes and peptidic azides and the subsequent copper-free thio acid/azide “sulfo-click” amidation reaction between the obtained dendrimeric peptide thio acids and a DOTA-derived sulfonyl azide (1). The ^111^In-labeling was achieved in NH_4_OAc buffer (pH 5.5) with ^111^InCl_3_ by heating the reaction mixture for 10–15 min at 95ºC. The radiochemical yield of the ^111^In-dimeric [Tyr^3^]octreotide was >98% with a specific activity of 22.7 GBq/μmol (0.61 Ci/μmol). Its lipophilicity, expressed as log(D) value, was −1.79 ± 0.11, more lipophilic than that of [^111^In-DOTA^0^,Tyr^3^]octreotide (−3.59 ± 0.14). This could be attributed to the aromatic character of the dendrimer-derived linker moiety.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20411957)]

Binding affinity of the dimeric [Tyr^3^]octreotide for SSTRs was determined using SSTR2-expressing AR42J tumor cells in a competitive binding assay (1). [^111^In-DOTA^0^,Tyr^3^]octreotide was used as a radiotracer, and commercially available [DOTA^0^,Tyr^3^]octreotide was included as a competing ligand. The dimeric [Tyr^3^]octreotide had a 50% inhibition concentration (IC_50_) of 2.45 nM, comparable to that of the reference [DOTA^0^,Tyr^3^]octreotide (IC_50_ = 2.45 nM). The IC_50_ values for the monomeric and tetrameric [Tyr^3^]octreotide conjugates were 1.32 nM and 14.0 nM, respectively. These results showed a decreased binding affinity with increased valency. The hypothesized increase in receptor affinity due to multimerization was not observed, especially in the case of tetrameric [Tyr^3^]octreotide, which may be attributed to the limited water solubility of the [Tyr^3^]octreotide conjugates. The IC_50_ values for all ^111^In-labeled conjugates improved by a factor of 1.4–2.9, compared to unlabeled counterparts.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20411957)]

In vivo biodistribution and tumor targeting of ^111^In-dimeric [Tyr^3^]octreotide (0.37 MBq (0.01 mCi), 0.1 µg) were investigated in BALB/c nude mice bearing subcutaneous AR42J tumors (n = 5 mice/time point) (1). [^111^In-DOTA^0^,Tyr^3^]octreotide was used as the reference compound, with a tumor uptake of 19.5 ± 4.84% injected dose per gram tissue (ID/g) at 2 h and 7.47 ± 0.78% ID/g at 24 h after tail vein injection. ^111^In-Dimeric [Tyr^3^]octreotide exhibited a specific and high tumor uptake of 25.31 ± 5.86% ID/g at 2 h, 30.91 ± 6.61% ID/g at 6 h, and 10.75 ± 2.98% ID/g at 24 h after injection. High activity at 6 h after injection indicates a prolonged retention of this compound in the tumors. The tumor uptake could be blocked with co-injection of excess octreotide (50 µg, n = 3 mice) (decreased to 5.55 ± 0.43% ID/g at 2 h). The blood clearance of ^111^In-dimeric [Tyr^3^]octreotide was relatively fast (1.52 ± 0.36% ID/g at 2 h and 0.17 ± 0.01% ID/g at 24 h), with the tumor/blood ratios increasing from 16.7 at 2 h to 35.9 at 6 h and to 71 at 24 h after injection. Among the organs, the kidney had the highest uptake with 92.20 ± 13.08% ID/g, 65.61 ± 9.71% ID/g, and 11.74 ± 3.31% ID/g at 2 h, 6 h, and 24 h, respectively. Low uptake was observed in the pancreas, stomach, and colon. The higher tumor uptake of ^111^In-dimeric [Tyr^3^]octreotide compared to [^111^In-DOTA^0^,Tyr^3^]octreotide emphasizes the importance of the implemented sulfonamide linker and dendrimer-derived core for tumor targeting.

^111^In-Monomeric [Tyr^3^]octreotide (refer to MICAD chapter for details (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) exhibited behavior similar to ^111^In-dimeric [Tyr^3^]octreotide, whereas ^111^In-tetrameric [Tyr^3^]octreotide behaved differently than its monomeric and dimeric counterparts. ^111^In-Tetrameric [Tyr^3^]octreotide had high uptake in the liver and spleen, but negligible tumor accumulation. Tetramerization of the [Tyr^3^]octreotide had profound implications on its lipophilicity and consequently on receptor affinity and tumor uptake.

In conclusion, the IC_50_ values of mono- and multimeric [Tyr^3^]octreotide conjugates are all in the low nanomolar range. Monomeric [Tyr^3^]octreotide has the highest binding affinity for SSTRs, followed by dimeric [Tyr^3^]octreotide and tetrameric [Tyr^3^]octreotide. In mouse models, ^111^In-monomeric [Tyr^3^]octreotide shows the highest tumor uptake, better than that of the [^111^In-DOTA^0^,Tyr^3^]octreotide, whereas ^111^In-dimeric [Tyr^3^]octreotide exhibits the longest tumor retention, probably due to the bivalency effect. Both monomeric and dimeric [Tyr^3^]octreotide conjugates exhibit interesting properties for imaging and therapeutic applications (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Yim C.B., Dijkgraaf I., Merkx R., Versluis C., Eek A., Mulder G.E., Rijkers D.T., Boerman O.C., Liskamp R.M. (2010). Synthesis of DOTA-conjugated multimeric [Tyr3]octreotide peptides via a combination of Cu(I)-catalyzed "click" cycloaddition and thio acid/sulfonyl azide "sulfo-click" amidation and their in vivo evaluation. J Med Chem.
2 Tulipano G., Schulz S. (2007). Novel insights in somatostatin receptor physiology. Eur J Endocrinol.
3 Lesche S., Lehmann D., Nagel F., Schmid H.A., Schulz S. (2009). Differential effects of octreotide and pasireotide on somatostatin receptor internalization and trafficking in vitro. J Clin Endocrinol Metab.
4 van der Hoek J., Hofland L.J., Lamberts S.W. (2005). Novel subtype specific and universal somatostatin analogues: clinical potential and pitfalls. Curr Pharm Des.
5 Strowski M.Z., Blake A.D. (2008). Function and expression of somatostatin receptors of the endocrine pancreas. Mol Cell Endocrinol.
6 Froidevaux S., Eberle A.N. (2002). Somatostatin analogs and radiopeptides in cancer therapy. Biopolymers.
7 Kwekkeboom D.J., Kam B.L., van Essen M., Teunissen J.J., van Eijck C.H., Valkema R., de Jong M., de Herder W.W., Krenning E.P. (2010). Somatostatin-receptor-based imaging and therapy of gastroenteropancreatic neuroendocrine tumors. Endocr Relat Cancer.
8 de Jong M., Breeman W.A., Kwekkeboom D.J., Valkema R., Krenning E.P. (2009). Tumor imaging and therapy using radiolabeled somatostatin analogues. Acc Chem Res.
9 Bal C.S., Gupta S.K., Zaknun J.J. (2010). Radiolabeled somatostatin analogs for radionuclide imaging and therapy in patients with gastroenteropancreatic neuroendocrine tumors. Trop Gastroenterol.
10 Ferone D., Saveanu A., Culler M.D., Arvigo M., Rebora A., Gatto F., Minuto F., Jaquet P. (2007). Novel chimeric somatostatin analogs: facts and perspectives. Eur J Endocrinol.
11 Hofland, L.J., J. van der Hoek, R. Feelders, A.J. van der Lely, W. de Herder, and S.W. Lamberts, Pre-clinical and clinical experiences with novel somatostatin ligands: advantages, disadvantages and new prospects. J Endocrinol Invest, 2005. 28(11 Suppl International): p. 36-42.
12 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
13 Gerasimou G., Moralidis E., Gotzamani-Psarrakou A. (2010). Somatostatin receptor imaging with (111)In-pentetreotide in gastro-intestinal tract and lung neuroendocrine tumors-Impact on targeted treatment. Hell J Nucl Med.
14 Mintzer, M.A. and M.W. Grinstaff, Biomedical applications of dendrimers: a tutorial. Chem Soc Rev, 2010